# 1-(2-[^18^F]Fluoro-3-pyridyl)-4-(2-propyl-1-oxo-isoindoline-5-yl)-5-methyl-1H-1,2,3-triazole

Chemical name: | 1-(2-[^18^F]Fluoro-3-pyridyl)-4-(2-propyl-1-oxo-isoindoline-5-yl)-5-methyl-1H-1,2,3-triazole
Abbreviated name: | [^18^F]MK-1312
Synonym:
Agent category: | Compound
Target: | Metabotropic glutamate receptor subtype 1 (mGluR1)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MK-1312)]

Glutamate is a major excitatory neurotransmitter at neuronal synapses in the central nervous system (CNS) (1, 2). Glutamate produces its excitatory effects by acting on cell-surface ionotropic glutamate or metabotropic glutamate receptors (mGluRs). The mGluRs are GTP-binding protein (G-protein)–coupled receptors that play important roles in regulating the activity of many synapses in the CNS, and many neuronal projection pathways contain mGluRs. There are eight mGluR subtypes, which are further subdivided into groups I, II, and III. The group I receptors include mGluR1 and mGluR5, and they are found predominantly in postsynaptic locations. The mGluR1 is found in moderate to high density in the cerebellum, caudate, putamen, thalamus, cingulate cortex, and hippocampus, with low density in the pons. The mGluR5 is usually found in moderate to high density in the frontal cortex, caudate, putamen, nucleus accumbens, olfactory tubercle, and hippocampus, whereas the density in the cerebellum is low. The mGluR1 and mGluR5 are positively coupled to phospholipase C in the regulation of neuronal excitability (3). Dysfunction of mGluR1 and mGluR5 is implicated in a variety of diseases in the CNS, including anxiety, depression, schizophrenia, Parkinson’s disease, and drug addiction or withdrawal (2, 4).

Positron emission tomography (PET) and single-photon emission tomography of radioligands targeting the mGluR1 can visualize and analyze mGluR1 expression in normal physiological and pathological conditions. Several radioligands have been studied for in vivo imaging of the mGluR1 in the brain (5). 1-(2-Fluoro-3-pyridyl)-4-(2-propyl-1-oxo-isoindoline-5-yl)-5-methyl-1H-1,2,3-triazole (MK-1312) was shown to be selective for the mGluR1, with nanomolar affinity (3.6 nM), and exhibited little inhibition of the mGluR5 (6). Hostetler et al. (6) prepared and evaluated 1-(2-[^18^F]fluoro-3-pyridyl)-4-(2-propyl-1-oxo-isoindoline-5-yl)-5-methyl-1H-1,2,3-triazole ([^18^F]MK-1312) for use with in vivo PET imaging of mGluR1 distribution in the brain of rhesus monkeys.

### Related Resource Links:

- Chapters in MICAD (mGluR1 (http://www.ncbi.nlm.nih.gov/books?Db=books&Cmd=DetailsSearch&Term=mGluR1+AND+micad%5Bbook%5D), mGluR5 (http://www.ncbi.nlm.nih.gov/books?term=mGluR5%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (mGluR1 (http://www.ncbi.nlm.nih.gov/gene/2911), mGluR5 (http://www.ncbi.nlm.nih.gov/gene/2915))
- Articles in Online Mendelian Inheritance in Man (OMIM) (mGluR1 (http://omim.org/entry/604473), mGluR5 (http://www.ncbi.nlm.nih.gov/omim/604102))
- Clinical trials (mGluR1 (http://www.clinicaltrials.gov/ct2/results?term=mGluR1), mGluR5 (http://www.clinicaltrials.gov/ct2/results?term=mglur5))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MK-1312%20and%20synthesis)]

Hostetler et al. (6) reported a one-step automated synthesis of [^18^F]MK-1312. The chloro-precursor was subjected to nucleophilic fluorination with K[^18^F]F/Kryptofix2.2.2 for 4 min at 120°C, with a radiochemical yield of 46 ± 15% and an average specific activity of 91.39 ± 51.43 GBq/µmol (2.47 ± 1.39 Ci/µmol, n = 25) after purification with high-performance liquid chromatography. The radiochemical purity of [^18^F]MK-1312 was >98%. The total synthesis time was ~45 min. MK-1312 exhibited a log P value of 2.3.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MK-1312%20and%20in%20vitro)]

In vitro [^18^F]MK-1312 autoradiography studies were performed on rhesus monkey and human brain sections (n = 6/group) (6). [^18^F]MK-1312 bound heterogeneously to the brain sections of both species, with the highest accumulation of radioactivity in the mGluR1-rich cerebellum, followed by a moderate radioactivity in the hippocampus and thalamus, and with the lowest radioactivity in the cortical regions and caudate/putamen. MK-1312 or MK-5435 (10,000 nM, mGluR1 antagonists) completely blocked radioactive signals to background levels in these brain regions. Saturation binding studies using [^18^F]MK-1312 with monkey and human cerebellum and cortex homogenates were performed. The binding potential (BP, B_max_/K_d_) values were 20 and 132 for the monkey cortex and cerebellum, respectively. The BP values were 24 and 98 for the human cortex and cerebellum, respectively. There was one binding site for the monkey brain homogenates and one for the human brain homogenates, with K_d_ values of 0.45 ± 0.13 nM and 0.97 ± 0.29 nM, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MK-1312%20and%20rodentia)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MK-1312%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MK-1312%20and%20%28primate%20not%20human%29)]

Hostetler et al. (6) performed dynamic PET imaging studies for 90 min in rhesus monkeys (n = 2) after intravenous injection of [^18^F]MK-1312. Baseline tissue time-activity curves revealed a high accumulation of radioactivity in the cerebellum, with lower accumulation of radioactivity in the thalamus and striatum. The maximum standard uptake values (SUVs) were 2.5, 2.0, and 2.1 for the cerebellum, thalamus, and striatum, respectively. [^18^F]MK-1312 remained 17% intact in the plasma at 90 min. Receptor occupancy was determined by administration of a bolus injection (0.015–0.45 mg/kg) plus infusion of MK-5435 (0.0075–0.2 mg/kg per h) for 60 min before injection of [^18^F]MK-1312. MK-5435 showed a dose-dependent reduction of radioactivity in all brain regions. The highest dose of MK-5435 was used to determine mGluR1 receptor occupancy in the cerebellum. The Hill constant was 0.84 ± 0.06, and 50% occupancy was 76 ± 7 nM (n = 7).

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MK-1312%20and%20human)]

No publication is currently available.

## References

1 Pin J.P., Duvoisin R. (1995). The metabotropic glutamate receptors: structure and functions. Neuropharmacology.
2 Ferraguti F., Crepaldi L., Nicoletti F. (2008). Metabotropic glutamate 1 receptor: current concepts and perspectives. Pharmacol Rev.
3 Abe T., Sugihara H., Nawa H., Shigemoto R., Mizuno N., Nakanishi S. (1992). Molecular characterization of a novel metabotropic glutamate receptor mGluR5 coupled to inositol phosphate/Ca2+ signal transduction. J Biol Chem.
4 Gasparini F., Lingenhohl K., Stoehr N., Flor P.J., Heinrich M., Vranesic I., Biollaz M., Allgeier H., Heckendorn R., Urwyler S., Varney M.A., Johnson E.C., Hess S.D., Rao S.P., Sacaan A.I., Santori E.M., Velicelebi G., Kuhn R. (1999). 2-Methyl-6-(phenylethynyl)-pyridine (MPEP), a potent, selective and systemically active mGlu5 receptor antagonist. Neuropharmacology.
5 Yamasaki T., Fujinaga M., Yoshida Y., Kumata K., Yui J., Kawamura K., Hatori A., Fukumura T., Zhang M.R. (2011). Radiosynthesis and preliminary evaluation of 4-[18F]fluoro-N-[4-[6-(isopropylamino)pyrimidin-4-yl]-1,3-thiazol-2-yl]-N-methylb enzamide as a new positron emission tomography ligand for metabotropic glutamate receptor subtype 1. Bioorg Med Chem Lett.
6 Hostetler E.D., Eng W., Joshi A.D., Sanabria-Bohorquez S., Kawamoto H., Ito S., O'Malley S., Krause S., Ryan C., Patel S., Williams M., Riffel K., Suzuki G., Ozaki S., Ohta H., Cook J., Burns H.D., Hargreaves R. (2011). Synthesis, characterization, and monkey PET studies of [(1)(8)F]MK-1312, a PET tracer for quantification of mGluR1 receptor occupancy by MK-5435. Synapse.